# ^64^Cu-DTPA-CLIO-VT680

Chemical name: | ^64^Cu-DTPA-CLIO-VT680
Abbreviated name: | ^64^Cu-TNP
Synonym: | ^64^Cu trireporter nanoparticle
Agent Category:
Target: | Macrophages
Target Category: | Phagocytosis
Method of detection: | Magnetic resonance imaging (MRI), optical, positron emission tomography (PET)
Source of signal/contrast: | Iron oxides, VT680, ^64^Cu
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=64Cu + trireporter)]

Macrophages are key cellular mediators of inflammation in atheroma and participate in all phases of atherogenesis (1, 2). The atheroma lesion is initialized by recruiting monocytes in inflamed intima. Monocytes mature into macrophages under the in situ stimulation of overexpressed macrophage colony-stimulating factor. As cholesteryl esters gradually accumulate in cytoplasm, macrophages are converted into foam cells at the early stage of atheroma. The accumulation of foam cells leads to the formation of fatty streaks and the deposition of fibrous tissues, indicating the progression of atheroma into an intermediate stage. Fibrous caps are formed on the surface of a lipid-rich core and result in vulnerable plaque as the smooth muscle cells synthesize bulk extracellular matrix. The rupture of plaque and the calcification of vessel walls progressively occlude the lumen. All of these developmental stages are produced in apolipoprotein E–deficient (apoE^-/-^) mice (3), a transgenic animal model with targeted deletion of the apoE gene. As a ligand, apoE binds to the receptors that are responsible for clearing chylomicrons and very low density lipoprotein remnants (4). A deficiency in apoE reduces diet cholesterol absorption and leads to a substantial increase in plasma cholesterol levels. ApoE^-/-^ mice are used in the study of spontaneous hypercholesterolemia and the subsequent development of atherosclerotic lesions (4, 5). The histopathological progression found in apoE^-/-^ mice is very similar to that found in humans (3). Because the arch shape and the proximity to three major arteries (the right and left common carotid arteries and the left subclavian arteries), atherosclerosis primarily occurs at the aortic arch in apoE^-/-^ mice (3).

Dextran-coated paramagnetic nanoparticles, such as ultra-small superparamagnetic iron oxide particles (USPIO), are known to accumulate in the macrophages located in inflamed lesions and carotid artery plaques after intravenous administration (6). The active internalization mechanism may be associated with dextran receptor–mediated endocytosis (1). Intracellular dextranase cleaves the dextran coating and leaves the iron oxide to be solubilized into iron ions followed by progressive incorporation into the hemoglobin pool (6). Because of long circulation times, excellent biocompatibility, and high relaxivity, USPIO are widely used to enhance magnetic resonance imaging (MRI) contrast for imaging lesional macrophages in stroke, multiple sclerosis, atherosclerotic diseases, spinal cord injury, and brain tumors (6). Monocrystalline iron oxide nanoparticles (MION) are a special type of USPIO that contain an icosahedral core of superparamagnetic crystalline Fe_3_O_4_ (magnetite) with a diameter of ~5 nm (7). Using epichlorohydrin to cross-link the dextran coating and amine groups to functionalize the surface, MION can be converted into an aminated platform (cross-linked iron oxide (CLIO)-NH_2_) that allows attachment of various imaging probes (8). CLIO-NH_2_ carrying fluorescent probes has demonstrated preferential uptake by lesional macrophages, concomitant with a much lower uptake by endothelial cells and smooth muscle cells (1).

^64^Cu-Labeled diethylenetriamine pentaacetic acid (DTPA)-CLIO-Vivotag 680 (VT680) is a ^64^Cu-labeled triple reporter nanoparticle (^64^Cu-TNP) used in MRI, positron-emission tomography (PET), and optical fluorescence imaging (9). ^64^Cu-TNP consists of three probe types. A CLIO-NH_2_ forms the core of the nanoparticle, generates a T_2_-shortening effect in MRI, and is recognizable by macrophages. Numerous complexes of ^64^Cu-DTPA are attached to the surface of CLIO-NH_2_ for PET detection. ^64^Cu is a positron-emitting radionuclide with an intermediate half-life (12.7 h) that decays by positron (β^+^) with a branching factor of 17.4% and a maximum β^+^ energy of 0.653 MeV (10). ^64^Cu has been used as a radiotracer in PET imaging and a radiotherapy agent in cancer treatment. Five molecules of VT680, an amine-reactive N-hydroxysuccinimide (NHS) ester of a (benzyl)-indolium–derived far-red fluorescent probe that remains internalized in cells for days without interfering with cell functions, are attached to CLIO-NH_2_ for fluorescence imaging (11). Its excitation/emission peak is located at 670 ± 5 nm/688 ± 5 nm. The internalization mechanism includes diffusion into cells within minutes and covalent binding to cellular components (11). This macrophage-targeted PET/MRI/optical agent allows complementary information to be obtained by multimodal imaging (9). The PET tracer is detected at 10^-6^–10^-8^ M (10), providing a sensitivity to detection that is at least one order of magnitude higher than the 10^-5^ M in MRI (9). The spatial resolution of MRI permits mapping of the atherosclerotic vascular territories. The cell-specified optical probes explore the fate of the imaging probe at cellular levels (9, 11).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + trireporter)+AND+synthesis%0D%0A)]

Nahrendorf et al. described a detailed synthesis of ^64^Cu-TNP (9). As the core of the triple reporter agent, CLIO-NH_2_ was synthesized in several steps (12). The starting material MION was synthesized by neutralization of ferrous salts, ferric salts, and dextran with ammonium hydroxide, followed by ultra-filtration. The obtained MION was cross-linked in a strong base with epichlorohydrin and then reacted with ammonia to produce CLIO-NH_2_. CLIO-NH_2_ then was reacted with the NHS ester of VT680 (commercially available) followed by incubation with excess dianhydride DTPA. Finally, the purified product was reacted with 185 MBq (0.5 mCi) ^64^CuCl_2_. For MRI experiments, stable nonradioactive copper salts (CuCl_2_) were used to produce Cu-TNP. ^64^Cu-TNP had a hydrodynamic diameter of ~20 nm and was attached with five VT680 moieties per nanoparticle. The specific activity of ^64^Cu-TNP was determined to be 1 mCi per 0.1 mg Fe of the nanoparticles, corresponding to ~300 μCi per mouse at a dose of 1.5 mg Fe/kg.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + trireporter)+AND+%22in+vitro%22)]

The relaxation efficacy of Cu-TNP was measured at 0.47 T and 39°C (9). The T_1_ and T_2_ relaxivity values were found to be 29 and 60 mM^-1^s^-1^, respectively. The detectable threshold of Cu-TNP in MRI or PET was examined in an agar phantom (9) in which ^64^Cu-TNP was diluted in 2% agarose to concentrations ranging from 0.0025–10 mg Fe/ml. The phantom was imaged with a combined PET/computed tomography (CT) scan followed by MRI at 7 T. The detection threshold of ^64^Cu-TNP was found to be 0.1 μg Fe/ml in PET and 5 μg Fe/ml in MRI.

The efficiency of fluorescent labeling was examined in excised aortas with ex vivo fluorescence reflectance imaging at 700 nm (9). Mice were killed after MRI to obtain aorta tissue samples. With a magnification of ×2, the plaque target/background ratio was found to be 8.0 ± 1.9 in the aortic root, arch, and carotid arteries of ApoE^-/-^ mice. The excised aortas of apoE^-/-^ mice were digested in cell suspensions for flow cytometry study to determine the uptake of ^64^Cu-TNP at cellular levels (9). Fluorescein isothiocyanate–labeled monoclonal antibodies were used to identify macrophages, neutrophils, smooth muscle cells, and endothelial cells. Macrophage-associated activity was found to contribute 73.9% of the overall activity; other cells such as neutrophils, endothelial cells, lymphocytes, and smooth muscle cells also ingested ^64^Cu-TNP and collectively contributed the remaining signal activity (~26%). The aortic roots of apoE^-/-^ mice were also stained with hematoxylin and eosin for immunofluorescence imaging of cell nuclei (9). With an upright epifluorescence microscope, fluorescence images were obtained in three spectrally resolved channels: ultraviolet for 4',6-diamidino-2-phenylindole (DAPI) nuclear staining, Texas red for immunofluorescent cell-specific antibodies, and far-red for VT680. The primary accumulation of ^64^Cu-TNP appeared to be within macrophages, as demonstrated by co-localization with MAC-3 antigen. Some uptake also occurred in lesional smooth muscle cells adjacent to macrophage-rich regions of highly inflamed plaques and in endothelial cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + trireporter) +AND++rodentia)]

The blood half-life of ^64^Cu-TNP was measured in wild-type B6 mice (n=5) (9). Repetitive retro-orbital bleeds were collected at 0.5, 1, 2, 6, and 24 h after intravenous injection of 150 μCi ^64^Cu-TNP. The mean blood half-life of ^64^Cu-TNP was found to be 259 ± 39 min. The distribution ^64^Cu-TNP in various organs was examined 24 h after injection; at this time point, 81.3 ± 3.3% of activity (decay-corrected) remained in the animal. The percent injected dose per gram of tissue was 33.6 ± 7.3 in the liver, 15.8 ± 2.8 in the small intestine, 13.8 ± 1.8 in the kidney, 11.0 ± 2.5 in the lung, 9.4 ± 3.6 in the spleen, 6.0 ± 0.9 in the heart, 5.2 ± 0.9 in the aorta, 4.3 ± 1.1 in the lymph nodes, 2.4 ± 1.2 in the thymus, and 1.1 ± 0.3 in fat. In apoE^-/-^ mice, the organ distribution was similar to that found in the wild-type mice, but the percent injected dose was much higher than that found in wild-type mice: 260% in aortas and 392% in carotid arteries. No in vivo analysis of free ^64^Cu was performed.

ApoE^-/-^ mice (45 weeks old) on a 20-week, high-cholesterol diet were imaged with PET/CT(n=9) or MRI (n=5) (9). ApoE^-/-^ mice received intravenous injections of 303 ± 39 μCi ^64^Cu-TNP at a dose of 1.5 mg Fe/kg and were imaged with PET/CT 24 h later. This dose was approximately one order of magnitude lower than the 30 mg Fe/kg used in MRI. A solution containing 61% Iopamidol (a CT contrast agent) was infused continuously and intravenously at 65 μl/min during the 2-min CT acquisition, which was used to provide appropriate intravascular contrast at a spatial resolution of 72 μm. After completion of CT acquisition, a PET scan was performed for 30–45 min at a spatial resolution of 2 mm. All imaged apoE^-/-^ mice showed a significant PET signal in the aortic root and arch. The target/background ratio was 5.1 ± 0.9 in the aortic root. ^18^F-Fluoro-2-deoxy-D-glucose (^18^F-FDG) PET was used to further confirm the plaques in the aortic root regions. In vivo MRI studies were performed at 7 T. ApoE^-/-^ mice were imaged before and 48 h after intravenous injection of 30 mg Fe/kg Cu-TNP, using a gradient-echo fast and low angle shot (FLASH) sequence. A significant contrast enhancement was found in the aortic root 48 h after injection of Cu-TNP. After MRI, ex vivo fluorescence reflectance imaging and autoradiography were conducted on excised aortas to confirm the uptake of ^64^Cu-TNP.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + trireporter) +AND+(primate+non+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=(64Cu + trireporter) +AND+human)]

No publication is currently available.

### NIH Support

HL 080731, HL 078641, CA 92782

## References

1 Jaffer F.A., Libby P., Weissleder R. (2006). Molecular and cellular imaging of atherosclerosis: emerging applications. J Am Coll Cardiol.
2 Packard R.R., Libby P. (2008). Inflammation in atherosclerosis: from vascular biology to biomarker discovery and risk prediction. Clin Chem.
3 Coleman R., Hayek T., Keidar S., Aviram M. (2006). A mouse model for human atherosclerosis: long-term histopathological study of lesion development in the aortic arch of apolipoprotein E-deficient (E0) mice. Acta Histochem.
4 Meir K.S., Leitersdorf E. (2004). Atherosclerosis in the apolipoprotein-E-deficient mouse: a decade of progress. Arterioscler Thromb Vasc Biol.
5 Breslow J.L. (1996). Mouse models of atherosclerosis. Science.
6 Corot C., Petry K.G., Trivedi R., Saleh A., Jonkmanns C., Le Bas J.F., Blezer E., Rausch M., Brochet B., Foster-Gareau P., Baleriaux D., Gaillard S., Dousset V. (2004). Macrophage imaging in central nervous system and in carotid atherosclerotic plaque using ultrasmall superparamagnetic iron oxide in magnetic resonance imaging. Invest Radiol.
7 Shen T., Weissleder R., Papisov M., Bogdanov A., Brady T.J. (1993). Monocrystalline iron oxide nanocompounds (MION): physicochemical properties. Magn Reson Med.
8 Josephson L., Perez J.M., Weissleder R. (2001). Magnetic nanosensors for the detection of oligonucleotide sequences. Angew. Chem. Int. Ed. Engl.
9 Nahrendorf M., Zhang H., Hembrador S., Panizzi P., Sosnovik D.E., Aikawa E., Libby P., Swirski F.K., Weissleder R. (2008). Nanoparticle PET-CT imaging of macrophages in inflammatory atherosclerosis. Circulation.
10 McQuade P., Martin K.E., Castle T.C., Went M.J., Blower P.J., Welch M.J., Lewis J.S. (2005). Investigation into 64Cu-labeled Bis(selenosemicarbazone) and Bis(thiosemicarbazone) complexes as hypoxia imaging agents. Nucl Med Biol.
11 Swirski F.K., Berger C.R., Figueiredo J.L., Mempel T.R., von Andrian U.H., Pittet M.J., Weissleder R. (2007). A near-infrared cell tracker reagent for multiscopic in vivo imaging and quantification of leukocyte immune responses. PLoS ONE.
12 Wunderbaldinger P. Josephson L. Weissleder R. Crosslinked iron oxides (CLIO): a new platform for the development of targeted MR contrast agents Acad Radiol 2002 9Suppl 2S304 6 12188255